# ^124^I-Labeled anti-HER2-specific C6.5 diabody

Chemical name: | ^124^I-Labeled anti-HER2-specific C6.5 diabody
Abbreviated name: | ^124^I-C6.5db
Synonym:
Agent category: | Diabody, antibody fragment
Target: | Epidermal growth factor receptor (EGFR, HER2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^124^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=C6.5%20diabody)]

Epidermal growth factor (EGF) is a cytokine of 53 amino acids (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non–small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Single-chain variable fragments (scFvs) of antibodies with a molecular mass of 25 kDa are cleared very rapidly from the circulation, but they exhibit poor tumor retention because they have a lower affinity than the parent antibody (11). On the other hand, bivalent antibody fragments possess better tumor-targeting characteristics, including rapid tissue penetration, high target retention, and rapid blood clearance. The diabody (db) fragment (a dimer of scFvs; molecular mass, 52–55 kDa) has been evaluated for targeting in several tumor antigen systems and has demonstrated rapid tumor localization and high-contrast imaging (11, 12). In particular, C6.5db was constructed using the human anti-HER2 C6.5 scFv and radiolabeled with ^124/125^I for in vivo imaging of HER2 expression in tumors (13). C6.5db binds to an epitope of HER2 distinct from that bound by trastuzumab.

### Related Resource Links:

- Chapters in MICAD (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064))
- Articles in Online Mendelian Inheritance in Man (OMIM) (HER2 (http://www.ncbi.nlm.nih.gov/omim/?term=HER2))
- Clinical trials (HER2 imaging (http://www.clinicaltrials.gov/ct2/results?term=HER2+imaging))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=C6.5%20diabody%20and%20synthesis)]

C6.5db (11.1 nmol) was incubated with 370 MBq (10 mCi) Na^124^I and Iodogen-coated glass beads for 5 min at room temperature (13). ^124^I-C6.5db was isolated with size-exclusion column chromatography, with a radiochemical purity of >93.5% and specific activities of 5–15.5 MBq/nmol (0.14–0.42 mCi/nmol). ^124^I-C6.5db exhibited immunoreactivity of 71%–73%. C6.5db and C6.5 scFv were also radiolabeled with Na^125^I in the presence of chloramine T with immunoreactivity values of 87.6% and 65.3%, respectively. The specific activities of ^125^I-C6.5db and ^125^I-C6.5 scFv were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=C6.5%20diabody%20and%20in%20vitro)]

Adams et al. (13) performed binding experiments with C6.5db and C6.5 scFv using a Biacore sensor chip immobilized with extracellular domain of HER2 (4,200 sites/µm^2^). The dissociation constants (K_d_) of C6.5db and C6.5 scFv were calculated to be 0.4 nM and 16 nM, respectively. C6.5db and C6.5 scFv exhibited retention half-life values (t_½_) of 43 min and 2 min, respectively. In vitro binding of biotinylated C6.5db and C6.5 scFv to SKOV-3 cells expressing HER2 (3,200–4,800 sites/µm^2^ on the cell surface) was determined with flow cytometry. C6.5db and C6.5 scFv exhibited t_½_ values of 5 h and 3 min, respectively. Reddy et al. (14) showed that C6.5db bound to an epitope on HER2 distinct from that bound by trastuzumab.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=C6.5%20diabody%20and%20rodentia)]

Adams et al. (13) performed ex vivo biodistribution studies of ^125^I-C6.5db (0.13 nmol) in severe combined immunodeficient (SCID) mice (n = 5/group) bearing SKOV-3 xenografts at 1, 4, 24, 48, and 72 h after injection. ^125^I-C6.5db exhibited a rapid equilibration phase (t_½_α = 0.67 h) and a slower elimination phase from circulation (t_½_β = 6.42 h). Accumulation values in the tumors were 6.9% injected dose/gram (ID/g), 10.1% ID/g, 6.5% ID/g, 2.4% ID/g, and 1.4% ID/g at 1, 4, 24, 48, and 72 h, respectively. Radioactivity values in the blood were 21.5% ID/ml, 6.7% ID/ml, 0.7% ID/ml, 0.1% ID/ml, and <0.1% ID/ml at these time points, respectively. Accumulation in normal tissues was less than that in the tumor at 24 h and later. As a comparison, ^125^I-C6.5 scFv was performed at 24 h after injection. Accumulation values were 1.0% ID/g, 0.04% ID/g, and 0.05% ID/ml in the tumor, liver, and blood, respectively. Reddy et al. (14) performed ex vivo biodistribution studies of ^125^I-C6.5db in SCID mice (n = 5/group) bearing tumors with different HER2 densities: SKOV-3 (1.0 × 10^6^/cell), MDA-MB361/DYT2 (3.7 × 10^5^/cell), and MDA-MB231 (2.3 × 10^4^/cell) with accumulation values of 1.91% ID/g, 1.11% ID/g, and 0.31% ID/g at 24 h after injection, respectively. ^125^I-C6.5db tumor accumulation correlated with the HER2 tumor density in tumors with high, moderate, and low HER2 expression. No blocking studies were performed.

Positron emission tomography (PET) imaging was performed in SCID mice (n = 7/group) bearing SKOV-3 tumors at 4, 8, 24, and 48 h after injection of ^124^I-C6.5db (14). The tumors were clearly visualized at 4 h after injection. There was a time-dependent increase in tumor/background signal. The stomach and thyroid were clearly visualized at 24 h and 48 h, respectively. Tumor accumulation (% ID/g) was quantitated with PET and ex vivo necropsy-based analysis: 9.8 ± 0.4 versus 11.3 ± 1.4 at 4 h, 9.4 ± 0.9 versus 10.3 ± 2.3 at 8 h, 5.7 ± 0.7 versus 6.1 ± 2.1 at 24 h, and 3.0 ± 0.1 versus 3.2 ± 0.6 at 48 h. The PET-based quantitation showed a strong correlation with the necropsy-based quantitation (R^2^ = 0.96). No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=C6.5%20diabody%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=C6.5%20diabody%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=C6.5%20diabody%20and%20human)]

No publication is currently available.

## NIH Support

CA 65559, CA06927, CA09035

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Wu A.M., Chen W., Raubitschek A., Williams L.E., Neumaier M., Fischer R., Hu S.Z., Odom-Maryon T., Wong J.Y., Shively J.E. (1996). Tumor localization of anti-CEA single-chain Fvs: improved targeting by non-covalent dimers. Immunotechnology.
12 Viti F., Tarli L., Giovannoni L., Zardi L., Neri D. (1999). Increased binding affinity and valence of recombinant antibody fragments lead to improved targeting of tumoral angiogenesis. Cancer Res.
13 Adams G.P., Schier R., McCall A.M., Crawford R.S., Wolf E.J., Weiner L.M., Marks J.D. (1998). Prolonged in vivo tumour retention of a human diabody targeting the extracellular domain of human HER2/neu. Br J Cancer.
14 Reddy S., Shaller C.C., Doss M., Shchaveleva I., Marks J.D., Yu J.Q., Robinson M.K. (2011). Evaluation of the anti-HER2 C6.5 diabody as a PET radiotracer to monitor HER2 status and predict response to trastuzumab treatment. Clin Cancer Res.